# ^124^I-Anti-PSCA 2B3 minibody

Chemical name: | ^124^I-Anti-PSCA 2B3 minibody
Abbreviated name: | ^124^I-2B3
Synonym:
Agent category: | Antibody
Target: | Prostate stem-cell antigen (PSCA)
Target category: | Antigen
Method of detection: | PET
Source of signal: | ^124^I
Activation: | No
Studies: | - In Vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=2909844), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=9367211) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=8000) for more information about PSCA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2B3%20minibody)]

Prostate stem-cell antigen (PSCA) is a cell-surface protein (123 amino acids) that is expressed in normal prostate tissue and overexpressed in prostate cancer tissues (1). PSCA expression is detected in >80% of patients with local disease including high expression in bone metastases (2). Elevated levels of PSCA are correlated with increased tumor stage, grade, and androgen independence (3). PSCA overexpression is also observed in bladder and pancreatic cancers (4).

The anti-PSCA murine monoclonal antibody (mAb) 1G8 has been shown to have anti-tumor activity (5). A humanized version of the 1G8 mAb (hu1G8) has been radiolabeled as ^124^I-hu1G8 for tumor imaging in mice (6). However, it took ~1 week to observe an enhanced target/background ratio with positron emission tomography because of the slow kinetics of the mAb. A hu1G8 minibody fragment (2B3) (a dimer of scFvs-C_H_3 with a linker composed of 18 amino acids; molecular weight,~80 kDa) has been developed and labeled as ^124^I-2B3 minibody for tumor targeting studies (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+AND+2B3+synthesis)]

The 2B3 minibody was labeled with sodium [^124^I]iodide by the Iodogen method (7). ^124^I-2B3 was purified with gel filtration with specific activities of 5.6 ± 2.2 MBq/nmol (0.15 ± 0.06 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+in+vitro)]

Leyton et al. (7) reported the radioimmunoreactivity of the ^124^I-2B3 minibody for PSCA to be 32 ± 13% (n = 5) as determined by measuring ^124^I-2B3 minibody binding to SKW 6.4-PSCA cells. With the use of PSCA competition assays, binding affinity values were found to be 5 nM for 1G8, 25 nM for hu1G8, and 46 nM for 2B3 minibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+rodentia)]

Leyton et al. (7) performed biodistribution studies with ^124^I-2B3 minibody (~0.6 nmol/mouse) in nude mice bearing xenografts of the LAPC-9 (PSCA-positive) and PC-3 (PSCA-negative) tumor cell lines. The ^124^I-2B3 uptake in the LAPC tumors was 5.2 ± 1.6 percent of injected dose per gram (% ID/g) at 21 h after injection, whereas the uptake in the PC-3 tumors was 2.4 ± 0.2% ID/g at 21 h after injection. Accumulation of radioactivity in the lung, liver, spleen, and kidney was lower than in the tumors. PET imaging visualized the LPAC-9 tumor as early as 4 h after injection with a strong radioactivity signal in the abdomen area. At 21 h, the LAPC-9 tumor radioactivity signal (5.5% ID/g) was stronger than the signal in the abdomen area (2.0–4.1% ID/g) and the PC-3 tumors (2.9% ID/g). The fast blood and non-target tissue clearance pattern exhibited a half-life of 11.2 h during the elimination phase (β). ^124^I-Labeled control minibody showed only background radioactivity (0.6% ID/g) in the LPAC-9 tumors, but no blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I+2B3+and+human)]

No publication is currently available.

## NIH Support

CA92131, CA86306, P01 CA43904, CA16042

## References

1 Reiter R.E., Gu Z., Watabe T., Thomas G., Szigeti K., Davis E., Wahl M., Nisitani S., Yamashiro J., Le Beau M.M., Loda M., Witte O.N. (1998). Prostate stem cell antigen: a cell surface marker overexpressed in prostate cancer. Proc Natl Acad Sci U S A.
2 Lam J.S., Yamashiro J., Shintaku I.P., Vessella R.L., Jenkins R.B., Horvath S., Said J.W., Reiter R.E. (2005). Prostate stem cell antigen is overexpressed in prostate cancer metastases. Clin Cancer Res.
3 Gu Z., Thomas G., Yamashiro J., Shintaku I.P., Dorey F., Raitano A., Witte O.N., Said J.W., Loda M., Reiter R.E. (2000). Prostate stem cell antigen (PSCA) expression increases with high gleason score, advanced stage and bone metastasis in prostate cancer. Oncogene.
4 Amara N., Palapattu G.S., Schrage M., Gu Z., Thomas G.V., Dorey F., Said J., Reiter R.E. (2001). Prostate stem cell antigen is overexpressed in human transitional cell carcinoma. Cancer Res.
5 Gu Z., Yamashiro J., Kono E., Reiter R.E. (2005). Anti-prostate stem cell antigen monoclonal antibody 1G8 induces cell death in vitro and inhibits tumor growth in vivo via a Fc-independent mechanism. Cancer Res.
6 Olafsen T., Gu Z., Sherman M.A., Leyton J.V., Witkosky M.E., Shively J.E., Raubitschek A.A., Morrison S.L., Wu A.M., Reiter R.E. (2007). Targeting, imaging, and therapy using a humanized antiprostate stem cell antigen (PSCA) antibody. J Immunother.
7 Leyton J.V., Olafsen T., Lepin E.J., Hahm S., Bauer K.B., Reiter R.E., Wu A.M. (2008). Humanized radioiodinated minibody for imaging of prostate stem cell antigen-expressing tumors. Clin Cancer Res.